# ^17^O-Oxygen

Chemical name: | ^17^O-Oxygen
Abbreviated name: | ^17^O_2_
Synonym:
Agent category: | Compound
Target: | Oxygen metabolism
Target category: | Non-targeted
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | ^17^O
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Oxygen-17%20MRI)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear proton spins, the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) and other iron oxide formulations affect T2 primarily and lead to a decreased signal. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

The human brain (5% of total body weight) accounts for ~20% of total body oxygen consumption (2). Oxygen is consumed to produce water via oxidative phosphorylation and reoxidation of reduced molecules in the mitochondria. The cerebral rate of oxygen consumption (CMRO_2_) and the cerebral blood flow (CBF) are sensitive and quantitative indicators of the health of the brain. Reduced cerebral perfusion and oxygen consumption have been observed in neurodegenerative and cerebrovascular diseases. CMRO_2_ has been imaged using ^15^O positron emission tomography (PET) to monitor the H_2_^15^O concentration in the brain during inhalation of ^15^O_2_ (3, 4). However, ^15^O PET is not popular because of the short half-life (~2 min) of ^15^O, on-site generation of ^15^O_2_, and high background noise (^15^O_2_ bound to hemoglobin versus H_2_^15^O). CMRO_2_ has also been measured with ^17^O nuclear magnetic resonance (NMR) spectroscopy and MRI after inhalation of ^17^O_2_, which is converted to H_2_^17^O (5, 6). ^17^O cannot be detected because molecular ^17^O_2_ is dissolved in the blood or is bound to hemoglobin as ^17^O_2_. ^17^O is detectable as in H_2_^17^O. ^17^O decreases the proton T2 relaxation time of water as the direct method of NMR/MRI measurement. The other method is indirect MRI measurement based on the enhancement of T1p relaxation of protons in water by ^17^O. CMRO_2_ and CBF can be measured with ^17^O NMR spectroscopy and MRI after inhalation of ^17^O_2_. CBF can be measured with ^17^O NMR spectroscopy and MRI after injection of H_2_^17^O.

### Related Resource Links:

- Clinical trials (^15^O-water (http://www.clinicaltrials.gov/ct2/results?term=15O+water))
- ^15^O-water information in FDA (http://google2.fda.gov/search?q=15O-water&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=4&y=14)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Oxygen-17%20MRI%20+and+synthesis)]

^17^O_2_ and H_2_^17^O are available commercially. No details of their synthesis were reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Oxygen-17%20MRI+and+in+vitro)]

Zhu et al. (6) performed NMR measurement of T1 and T2 relaxation times of H_2_^17^O in saline solution at 4.7 T. The T1 and T2 values were 6.59 and 4.28 ms, respectively. The T1 and T2 values at 9.4 T were similar to those at 4.7 T.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Oxygen-17%20MRI+and+rodentia)]

Zhu et al. (7) performed NMR spectroscopy for fast imaging of CMRO_2_ in rat brain at 9.4 T during a short inhalation of ^17^O_2_. The CMRO_2_ and CBF values (n = 7) were found to be 2.19 ± 0.14 µmol/g/min and 0.53 ± 0.07 ml/g/min, respectively.

Tailor et al. (5) introduced ^17^O_2_ to rats using a closed respiration circuit delivery system. ^1^H T1p-weighted MRI was performed as indirect ^17^O imaging at 4 T. The CMRO_2_ value (n = 4) was estimated to be 2.10 ± 0.44 µmol/g/min.

Fiat et al. (8) estimated the CMRO_2_ value (n = 5) to be 2.09 ± 0.35 µmol/g/min with ^17^O NMR spectroscopy and imaging (7 T) during ^17^O_2_ inhalation in rats.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Oxygen-17%20MRI+and+(dog+or+sheep+or+pig+or+rabbit))]

Fiat et al. (8) estimated the CMRO_2_ value (n = 5) to be 1.18 ± 0.58 µmol/g/min with ^17^O NMR spectroscopy and imaging (4.7 T) during ^17^O_2_ inhalation in cats. The CBF value was estimated to be 0.38 ± 0.12 ml/g/min.

Pekar et al. (9) estimated the CMRO_2_ value (n = 7) to be 1.5 ± 0.05 µmol/g/min using ^1^H MRI measurement (4.7 T) during ^17^O_2_ inhalation in cats. The CBF value was estimated to be 0.38 ± 0.15 ml/g/min.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Oxygen-17%20MRI+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Oxygen-17%20MRI+and+human)]

Fiat et al. (10) performed ^17^O MRI mapping of one human brain at 1.5 T during ^17^O_2_ inhalation. The CMRO_2_ and CBF values were estimated to be ~1.4 µmol/g/min and ~0.6 ml/g/min, respectively.

Atkinson et al. (11) performed ^17^O MRI mapping of one human brain at 9.4 T during ^17^O_2_ inhalation. The CMRO_2_ values for the gray and white matter were estimated to be 1.42 ± 0.05 µmol/g/min and 0.75 ± 0.11 µmol/g/min, respectively. The CMRO_2_ value for the whole brain was found to be 1.18 µmol/g/min. These CMRO_2_ values are in agreement with 15O-PET published values (3, 4).

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Shulman R.G., Rothman D.L., Behar K.L., Hyder F. (2004). Energetic basis of brain activity: implications for neuroimaging. Trends Neurosci.
3 Leenders K.L., Perani D., Lammertsma A.A., Heather J.D., Buckingham P., Healy M.J., Gibbs J.M., Wise R.J., Hatazawa J., Herold S., et al. (1990). Cerebral blood flow, blood volume and oxygen utilization. Normal values and effect of age. Brain.
4 Mintun M.A., Raichle M.E., Martin W.R., Herscovitch P. (1984). Brain oxygen utilization measured with O-15 radiotracers and positron emission tomography. J Nucl Med.
5 Tailor D.R., Baumgardner J.E., Regatte R.R., Leigh J.S., Reddy R. (2004). Proton MRI of metabolically produced H2 17O using an efficient 17O2 delivery system. Neuroimage.
6 Zhu X.H., Merkle H., Kwag J.H., Ugurbil K., Chen W. (2001). 17O relaxation time and NMR sensitivity of cerebral water and their field dependence. Magn Reson Med.
7 Zhu X.H., Zhang Y., Tian R.X., Lei H., Zhang N., Zhang X., Merkle H., Ugurbil K., Chen W. (2002). Development of (17)O NMR approach for fast imaging of cerebral metabolic rate of oxygen in rat brain at high field. Proc Natl Acad Sci U S A.
8 Fiat D., Kang S. (1993). Determination of the rate of cerebral oxygen consumption and regional cerebral blood flow by non-invasive 17O in vivo NMR spectroscopy and magnetic resonance imaging. Part 2. Determination of CMRO2 for the rat by 17O NMR, and CMRO2, rCBF and the partition coefficient for the cat by 17O MRI. Neurol Res.
9 Pekar J., Sinnwell T., Ligeti L., Chesnick A.S., Frank J.A., McLaughlin A.C. (1995). Simultaneous measurement of cerebral oxygen consumption and blood flow using 17O and 19F magnetic resonance imaging. J Cereb Blood Flow Metab.
10 Fiat D., Hankiewicz J., Liu S., Trbovic S., Brint S. (2004). 17O magnetic resonance imaging of the human brain. Neurol Res.
11 Atkinson I.C., Thulborn K.R. (2010). Feasibility of mapping the tissue mass corrected bioscale of cerebral metabolic rate of oxygen consumption using 17-oxygen and 23-sodium MR imaging in a human brain at 9.4 T. Neuroimage.